# (-)-N-[^11^C]Propyl-norapomorphine

Chemical name: | (-)-N-[^11^C]Propyl-norapomorphine
Abbreviated name: | [^11^C]NPA
Synonym:
Agent category: | Compound
Target: | D_2_ dopamine receptors
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system level. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostiatal axons.

Dopamine receptors are G protein-coupled receptors and exist in high- and low- affinity states, with respect to agonist binding. The two states are interconvertible. The high-affinity state is coupled to G-proteins, whereas the low-affinity state is not. Dopamine has a K_d_ of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiological conditions, dopamine is expected to bind predominately to the high-affinity state, which is ~50% occupied by 10 nM dopamine. The high-affinity state was suggested to be the functional form of the dopamine receptors.

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making studies of extrastriatal D_2_ receptors difficult (6-8). In binding studies, [^123^I]-labeled epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2_ receptors (9). Epidepride has marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (10), and in positron emission tomography (PET) in vivo studies (11-13), it identified extrastriatal D_2/3_ receptors. However, all these antagonists do not distinguish between the high- and low- affinity states of the D_2_ receptors. (-)-N-Propyl-norapomorphine (NPA), a full dopamine D_2/3_ receptor agonist, was reported to have the K_high_ and K_low_ values of 0.07-0.4 and 20-200 nM for D_2_ receptors, respectively (5, 14-16). This provides a >50-fold selectivity for the high-affinity over the low affinity receptors. It has good affinity (K_i_, 0.3 nM) for D_3_ receptors but not other neurotransmitters (17). [^11^C]NPA is being developed as a positron emission tomography (PET) agent for the non-invasive study of the high-affinity state of the D_2_ receptors in the brain.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D)
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in OMIM (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20synthesis)]

Hwang et al (18) reported an one-pot synthesis of [^11^C]NPA by reacting [^11^C]propionyl chloride with norapomorphine and a LiAlH_4_ reduction, with a radiochemical yield of 16% (based on [^11^C]CO_2_, end of bombardment) and an average specific activity of 63 GBq/μmol (1700 mCi/μmol at end of synthesis) after C-18 Sep-Pak and high-performance liquid chromatography (HPLC) purification. Radiochemical purities were >99%. [^11^C]Propionyl chloride was prepared by reacting [^11^C]CO_2_ with ethylmagnesium bromide, followed by reaction with phthaloyl chloride. The total synthesis time was 60 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20in%20vitro)]

In binding to dopamine receptors in membranes of porcine anterior pituitary, [^3^H]NPA had an average dissociation constant (K_d_) of 0.26 ± 0.01 nM and a B_max_ of 2.3 ± 0.1 pmol/g tissue (19). Guanilylimidodiphosphate completely inhibited [^3^H]NPA binding, suggesting that [^3^H]NPA was binding primarily to the high-affinity state of dopamine D_2_ receptors. Using [^3^H]spiroperidol, NPA had the K_high_ and K_low_ values of 0.27 ± 0.04 and 26 ± 2.6 nM, respectively, About 54% of D_2_ receptors were in the high-affinity state. Therefore, NPA has good selectivity and affinity for the high-affinity state of D_2_. George et al. (5) reported that NPA had the K_high_ and K_low_ values of 0.31 and 207 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20rodentia)]

Ex vivo biodistribution studies in rats showed a high accumulation of radioactivity in the kidney [1.00% injected dose (ID)/g], followed by liver (0.72% ID/g), adrenal (0.66% ID/g), lung (0.31% ID/g), and spleen (0.25% ID/g) at 5 min after injection of [^11^C]NPA (18). There was a marked accumulation of the tracer in the striatum within the first 30 min (0.88% ID/g), followed by a decrease of radioactivity to 0.56% ID/g at 60 min. The striatum/ cerebellum and frontal cortex/cerebellum ratios were 3.47 and 1.44 at 30 min after injection, respectively. Haloperidol pretreatment (1 mg/kg) effectively blocked specific binding of [^11^C]NPA to the striatum (from 0.88 to 0.28% ID/g) and frontal cortex (from 0.36 to 0.21% ID/g) at 30 min. Little inhibition was seen in the cerebellum (from 0.25 to 0.22% ID/g). [^11^C]NPA thus displays uptake and washout kinetics characteristic of reversible radiotracers.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20%28primate%20not%20human%29)]

[^11^C]NPA PET studies in non-human primates have provided useful assessment of the D_2_ receptor in the brain, showing localization of [^11^C]NPA in striatal regions. Hwang et al. (18) showed selective uptake in the striatum (0.031%ID/g) of a baboon monkey brain with striatum-to-cerebellum ratios of 2.33 at 15 min and 2.86 at 45 min after injection of 231 MBq (6.25 mCi) [^11^C]NPA. The striatal accumulation of [^11^C]NPA was inhibited by pretreatment with haloperidol (1 mg/kg) with the striatum-to-cerebellum ratio of 1.29 at 45 min after injection.

Hwang et al (20) performed quantitative measurements of [^11^C]NPA binding with kinetic and graphical analyses, using arterial input function to derive potential (BP) and specific-to-nonspecific equilibrium partition coefficient (V_3_”) in 2 baboons. In kinetic analyses, BP estimates were 4.04 ± 1.05 ml/g in the striatum, whereas BP estimates were 3.90 ± 1.03 ml/g using graphical analysis with arterial input. At 40 min post injection, 31% of [^11^C]NPA radioactivity remained intact in arterial plasma. It was concluded that data from 30 min of scanning were sufficient to derive V_3_” values by kinetic, graphical and simplified reference-tissue model analyses.

Narendran et al. (21) studied 3 male baboons with [^11^C]raclopride (a D_2_ antagonist) and [^11^C]NPA under baseline conditions and following administration of the potent DA releaser amphetamine . Kinetic modeling with an arterial input function was used to derive the striatal V_3_". [^11^C]Raclopride V_3_" was reduced by 24 ± 10%, 32 ± 6%, and 44 ± 9% following amphetamine doses of 0.3, 0.5, and 1.0 mg/kg, respectively. [^11^C]NPA V_3_" was reduced by 32 ± 2%, 45 ± 3%, and 53 ± 9% following amphetamine doses of 0.3, 0.5, and 1.0 mg/kg, respectively. Thus, endogenous DA was 42% more effective at competing with [^11^C]NPA binding compared to [^11^C]raclopride binding, which is consistent with the pharmacology of these tracers (agonist vs. antagonist). These results also suggest that 71% of D_2_ receptors are configured in a state of high affinity for agonists in vivo. [^11^C]NPA is able to detect the change in dopamine levels induced by D-amphetamine and is more vulnerable to competition by endogenous dopamine than that of antagonist radiotracer [^11^C]raclopride.

Narendran et al. (22) performed further PET studies in 3 baboons under noncarrier- and carrier-added conditions, to compare the B_max_ of [^11^C]NPA and [^11^C]raclopride in the same baboons. [^11^C]raclopride K_d_ and B_max_ were 1.59 ± 0.28 nM and 27.3 ± 3.9 nM, respectively. The in vivo K_d_ of [^11^C]NPA was 0.16 ± 0.01 nM, consistent with its affinity for D_2high_ reported in vitro binding. The B_max_ for [^11^C]NPA was 21.6 ± 2.8 nM and 79% of the [^11^C]raclopride B_max_. This result suggested that 79% of D_2_ receptors are configured as high-affinity state in vivo. This large proportion of high-affinity sites might explain the vulnerability of D_2_ radiotracers to competition by endogenous dopamine, and is consistent with the reported in vivo binding of agonist radiotracer [^11^C]NPA (21).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20human)]

Narendran et al. (23) studied the vulnerability of the in vivo binding of [^11^C]NPA to acute fluctuation in synaptic dopamine was assessed with PET imaging in ten healthy humans (eight females and two males) and compared with that of the reference D_2/3_ receptor antagonist radiotracer [^11^C]raclopride before and after the administration of 0.5 mg/kg oral d-amphetamine. The binding potential relative to nonspecific uptake (BP_ND_) values in the ventral striatum (VST), caudate (CAD), and putamen (PUT) were determined using kinetic modeling with an arterial input function. [^11^C]Raclopride BP_ND_ values were significantly reduced by 9.7 ± 4.4, 8.4 ± 4.2, and 14.7 ± 4.8% after amphetamine administration in the VST, CAD, and PUT, respectively. [^11^C]NPA BP_ND_ values were also reduced significantly by 16.0 ± 7.0, 16.1 ± 6.1, and 21.9 ± 4.9% after the same dose of amphetamine in the VST, CAD, and PUT, respectively. [^11^C]NPA was more vulnerable to endogenous competition by dopamine compared with [^11^C]raclopride by a factor of 1.49 - 1.90, which suggests that D_2/3_ agonist [^11^C]NPA is more vulnerable to endogenous competition by dopamine than D_2/3_ antagonist [^11^C]raclopride.

Lagmon et al. (24) performed dosimetry of [^11^C]NPA in 6 healthy subjects with PET scans after injection of 370 MBq (10 mCi). The highest organ dose was to the gallbladder wall, which received 2.81 x 10^–2^ mSv/MBq. An effective dose was 3.17 x 10^–3^ mSv/MBq.

## NIH Support

K08-MH068762, R21-DA023450, K02-MH01603-01, R01MH62089-01, MH59342-01

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 George S.R., Watanabe M., Di Paolo T., Falardeau P., Labrie F., Seeman P. (1985). The functional state of the dopamine receptor in the anterior pituitary is in the high affinity form. Endocrinology.
6 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
7 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
8 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
9 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
10 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
11 Grunder, G., C. Landvogt, I. Vernaleken, H.G. Buchholz, J. Ondracek, T. Siessmeier, S. Hartter, M. Schreckenberger, P. Stoeter, C. Hiemke, F. Rosch, D.F. Wong, and P. Bartenstein, The Striatal and Extrastriatal D2/D3 Receptor-Binding Profile of Clozapine in Patients with Schizophrenia. Neuropsychopharmacology, 2005
12 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
13 Riccardi, P., R. Li, M.S. Ansari, D. Zald, S. Park, B. Dawant, S. Anderson, M. Doop, N. Woodward, E. Schoenberg, D. Schmidt, R. Baldwin, and R. Kessler, Amphetamine-Induced Displacement of [(18)F] Fallypride in Striatum and Extrastriatal Regions in Humans. Neuropsychopharmacology, 2005
14 Gardner B., Strange P.G. (1998). Agonist action at D2(long) dopamine receptors: ligand binding and functional assays. Br J Pharmacol.
15 Lahti R.A., Mutin A., Cochrane E.V., Tepper P.G., Dijkstra D., Wikstrom H., Tamminga C.A. (1996). Affinities and intrinsic activities of dopamine receptor agonists for the hD21 and hD4.4 receptors. Eur J Pharmacol.
16 Seeman P., Watanabe M., Grigoriadis D., Tedesco J.L., George S.R., Svensson U., Nilsson J.L., Neumeyer J.L. (1985). Dopamine D2 receptor binding sites for agonists. A tetrahedral model. Mol Pharmacol.
17 Neumeyer J.L., Neustadt B.R., Oh K.H., Weinhardt K.K., Boyce C.B., Rosenberg F.J., Teiger D.G. (1973). Aporphines. 8. Total synthesis and pharmacological evaluation of (plus or minus)-apomorphine, (plus or minus)-apocodeine, (plus or minus)-N-n-propylnorapomorphine, and (plus or minus)-N-n-propylnorapocodeine. J Med Chem.
18 Hwang D.R., Kegeles L.S., Laruelle M. (2000). (-)-N-[(11)C]propyl-norapomorphine: a positron-labeled dopamine agonist for PET imaging of D(2) receptors. Nucl Med Biol.
19 Sibley D.R., De Lean A., Creese I. (1982). Anterior pituitary dopamine receptors. Demonstration of interconvertible high and low affinity states of the D-2 dopamine receptor. J Biol Chem.
20 Hwang D.R., Narendran R., Huang Y., Slifstein M., Talbot P.S., Sudo Y., Van Berckel B.N., Kegeles L.S., Martinez D., Laruelle M. (2004). Quantitative analysis of (-)-N-(11)C-propyl-norapomorphine in vivo binding in nonhuman primates. J Nucl Med.
21 Narendran R., Hwang D.R., Slifstein M., Talbot P.S., Erritzoe D., Huang Y., Cooper T.B., Martinez D., Kegeles L.S., Abi-Dargham A., Laruelle M. (2004). In vivo vulnerability to competition by endogenous dopamine: comparison of the D2 receptor agonist radiotracer (-)-N-[11C]propyl-norapomorphine ([11C]NPA) with the D2 receptor antagonist radiotracer [11C]-raclopride. Synapse.
22 Narendran R., Hwang D.R., Slifstein M., Hwang Y., Huang Y., Ekelund J., Guillin O., Scher E., Martinez D., Laruelle M. (2005). Measurement of the proportion of D2 receptors configured in state of high affinity for agonists in vivo: a positron emission tomography study using [11C]N-propyl-norapomorphine and [11C]raclopride in baboons. J Pharmacol Exp Ther.
23 Narendran R., Mason N.S., Laymon C.M., Lopresti B.J., Velasquez N.D., May M.A., Kendro S., Martinez D., Mathis C.A., Frankle W.G. (2010). A comparative evaluation of the dopamine D(2/3) agonist radiotracer [11C](-)-N-propyl-norapomorphine and antagonist [11C]raclopride to measure amphetamine-induced dopamine release in the human striatum. J Pharmacol Exp Ther.
24 Laymon C.M., Mason N.S., Frankle W.G., Carney J.P., Lopresti B.J., Litschge M.Y., Mathis C.A., Mountz J.M., Narendran R. (2009). Human biodistribution and dosimetry of the D2/3 agonist 11C-N-propylnorapomorphine (11C-NPA) determined from PET. J Nucl Med.